# 2-tert-Butyl-4-chloro-5-[4-(2-[^18^F]fluoro-ethoxymethyl)-benzyloxy]-3-(2H)-pyridazinone

Chemical name: | 2-tert-Butyl-4-chloro-5-[4-(2-[^18^F]fluoro-ethoxymethyl)-benzyloxy]-3-(2H)-pyridazinone
Abbreviated name: | [^18^F]MC1-27
Synonym:
Agent category: | Compound
Target: | Mitochondrial complex 1 (MC1)
Target category: | Enzyme
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20pyridazinone)]

Lipophilic cations are capable of passing through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to large negative plasma and mitochondrial membrane potentials. ^99m^Tc-2-Methoxyisobutylisonitrile (^99m^TcMIBI) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations, which are rapidly taken up into cells driven by mitochondrial metabolism and membrane potential (1-4). They are used as myocardial-perfusion single-photon emission computed tomography (SPECT) as well as tumor imaging agents. However, the high accumulation of technetium tracers in the lung and liver may interfere with the detection of flow abnormalities in the myocardium. More recently, positron emission tomography (PET) imaging has emerged as an alternative approach to evaluating myocardial blood flow by use of positron-emitting radionuclides (e.g. ^82^RbCl, ^13^NH_3_, and H_2_^15^O). However, the majority of these radiotracers exhibited short physical half-lives (<10 min). Lipophilic cations, such as [^11^C]triphenylmethylphosphonium ([^11^C]TPMP) (5) and 4-[^18^F]fluorobenzyl-triphenylphosphonium ([^18^F]FBnTP) have been investigated as PET agents for myocardial and tumor imaging (6).

Mitochondrial complex I (MC1) of the mammalian electron transfer chain is composed of at least 43 protein subunits, of which 7 are encoded by mitochondrial DNA (7). MC1 catalyzes the transfer of electrons from NADH to ubiquinone and translocates protons from the mitochondrial matrix to the intermembrane space to generate ATP and thereby the energy supply of the cell. MC1 may also play direct roles in the mitochondrial permeability transition and in cell death pathways. Myocardium has a high mitochondrial content because of high energy usage. 2-tert-Butyl-4-chloro-5-[4-(2-fluoro-ethoxymethyl)-benzyloxy]-3-(2H)-pyridazinone (MC1-27) is found to be a potent MC1 inhibitor with a hydrophobic heterocyclic chromone core (8). 2-tert-Butyl-4-chloro-5-[4-(2-[^18^F]fluoro-ethoxymethyl)-benzyloxy]-3-(2H)-pyridazinone ([^18^F]MC1-27) has been synthesized to study as a myocardium imaging PET agent.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Mitochondrial%20complex+AND+micad%5Bbook%5D)
- Gene information in NCBI (MC1 (http://www.ncbi.nlm.nih.gov/gene/291))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/252010)
- Clinical trials (MC1 (http://www.clinicaltrials.gov/ct2/results?term=Mitochondrial+complex+1+))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20pyridazinone+synthesis)]

[^18^F]MC1-27 was prepared as described by Purohit et al. (8). [^18^F]Fluoride/Kryptofix 2.2.2/K_2_CO_3_ and the tosylate precursor were heated in acetonitrile at 90°C for 30 min followed by high-performance liquid chromatography purification. Average radiochemical yield was 35% with a total synthesis time of 90 min. Radiochemical purity was >99% with specific activities of 27.8-74.0 GBq/µmol (0.75-2.0 Ci/µmol) at the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20pyridazinone%20and%20in%20vitro)]

Purohit et al. (8) reported that MC1-27 inhibited NADH oxidation (MC1) by bovine heart submitochondrial particles with an IC_50_ value of 11 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20pyridazinone%20and%20rodentia)]

Purohit et al. (8) performed ex vivo biodistribution studies of [^18^F]MC1-27 in rats. [^18^F]MC1-27 accumulated mainly in the heart with 3.41 ± 0.27% injected dose/g (ID/g) and 3.47 ± 0.37% ID/g at 30 and 120 min after injection, respectively. Retention of [^18^F]MC1-27 in the heart was good with no washout. The heart/blood, heart/lung, heart/liver and heart/femur ratios were 30.0, 16.1, 2.7, and 7.5 at 30 min after injection, respectively. The uptake in the femur was ~0.5% ID/g at 30 min indicating some defluorination of [^18^F]MC1-27. PET imaging showed that [^18^F]MC1-27 accumulated mainly in the heart and liver with low accumulation in the lung. Good myocardial images were observed at 25-35 min after injection and complete by 55-60 min with little interference from the lung and liver. Some bone uptake was observed in images after 30 min. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20pyridazinone+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20pyridazinone%20and%20%28primate%20not%20human%29)]

Purohit et al. (8) performed PET imaging studies of [^18^F]MC1-27 in male and female Rhesus monkeys. [^18^F]MC1-27 accumulated mainly in the heart within minutes after injection. Retention of [^18^F]MC1-27 in the heart was good with little washout, whereas the retention was much less in the liver. Accumulation of [^18^F]MC1-27 in the heart was clearly visualized over 120 min of imaging with no interference from the lung accumulation of [^18^F]MC1-27. No accumulation of [^18^F]MC1-27 in the bone was detected up to 120 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20pyridazinone%20and%20human)]

No publication is currently available.

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
4 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
5 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
6 Madar I., Ravert H.T., Du Y., Hilton J., Volokh L., Dannals R.F., Frost J.J., Hare J.M. (2006). Characterization of Uptake of the New PET Imaging Compound 18F-Fluorobenzyl Triphenyl Phosphonium in Dog Myocardium. J Nucl Med.
7 Lenaz G., Fato R., Genova M.L., Bergamini C., Bianchi C., Biondi A. (2006). Mitochondrial Complex I: structural and functional aspects. Biochim Biophys Acta.
8 Purohit A., Radeke H., Azure M., Hanson K., Benetti R., Su F., Yalamanchili P., Yu M., Hayes M., Guaraldi M., Kagan M., Robinson S., Casebier D. (2008). Synthesis and biological evaluation of pyridazinone analogues as potential cardiac positron emission tomography tracers. J Med Chem.